# Radioiodinated humanized monoclonal antibody A33

Chemical name: | Radioiodinated humanized monoclonal antibody A33
Abbreviated name: | Radioiodinated-huA33 mAb
Synonym: | [^125^I/^124^I/^131^I]huA33
Agent Category: | Humanized monoclonal antibody A33
Target: | Glycoprotein A33
Target Category: | Antibody-antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal / contrast: | ^125^I/^131^I
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click here for protein and nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=5031560) sequence of human A33 antigen.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=monoclonal+antibody+A33)]

The A33 cell-surface differentiation antigen is a glycoprotein that belongs to the immunoglobulin superfamily (1). This antigen is expressed in >95% of primary and metastatic colon cancer cells, but is absent in most normal and tumor cell types (2, 3). Although the exact function of this glycoprotein is unknown, antibodies developed against the A33 antigen bind to tumor cells and exhibit prolonged retention in the tumor tissue (4). The A33 antigen was considered an important target of a mouse monoclonal antibody (mAb) developed for the treatment of colorectal cancers; the radiolabeled mAb was detectable in the tumor tissue up to 6 weeks after administration, but it was cleared from normal tissue within a week (4, 5). Radioimmunotherapy studies in a nude mouse model also showed that the antitumor effects of the A33 antigen mAb were enhanced by combination with chemotherapeutic agents (6, 7). However, patients treated with the radioiodinated murine mAb A33 showed minimal gut toxicity but developed a human anti-mouse antibody (HAMA) response after the first treatment (8). On re-treatment, the radiolabeled antibody was rapidly cleared from the blood circulation of these patients, and on imaging the label was observed to have accumulated in the liver, spleen, or adrenals, but not at the tumor sites (8).

To reduce immunogenicity of the murine mAb, a humanized version of the A33 antibody (huA33) was constructed and is under evaluation in various clinical trials (http://clinicaltrials.gov/ct/search?term=huA33) (9-12). Recently huA33 was labeled with radioactive astatine (^211^At) or lutetium (^177^Lu) and studied for specificity, biodistribution, and tumor targeting in rodents (13, 14). From these studies it was concluded that the labeled antibody could be used for radioimmunotherapy of colorectal cancer.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33+antibody+synthesis)]

For some pre-clinical and clinical studies, a mouse mAb against glycoprotein A33 was produced as described by Welt et al. (5). Briefly, a mouse mAb A33 hybridoma cell line was derived by the fusion of spleen cells of BALB/c mice immunized with the AsPC-1 (http://www.biotech.ist.unige.it/cldb/cl289.html) pancreatic adenocarcinoma cell line and SP2/0 (http://www.biotech.ist.unige.it/cldb/cl4384.html) myeloma cells (15). The mAb was used either as a supernatant from the hybridoma cultures or purified from A33 hybridoma ascites (http://grants.nih.gov/grants/policy/antibodies.pdf) grown in pristine-treated and irradiated CByB6F1 mice as described elsewhere (4, 5, 8, 15). For clinical testing the antibody was tested according to standards set by the United States Food and Drug Administration (5).

The huA33 version of the antibody was produced in NSO (http://www.biotech.ist.unige.it/cldb/cl3738.html) cells as described by King et al. (9). A single plasmid was constructed to express the humanized heavy and light chains of mAb A33 and transfected into NSO cells to produce a stable cell line (9). The huA33 was purified from nitric oxide synthase supernatant by a three-step chromatographic procedure involving Q-Sepharose anion exchange, protein A affinity, and S-Sepharose cation exchange columns (12). The antibody was formulated in phosphate-buffered saline, sterile filtered, and stored at -70°C until required. The pure humanized mAb did not aggregate and had a binding specificity similar to the murine mAb (16).

Radioiodination of the murine mAb A33 was done with ^125^I/^131^I-labeled sodium iodide according to the chloramine-T method (17). The reaction was terminated with sodium metabisulphite, and the product was passed through a Sephadex G25 column to remove excess radioactivity. Fractions containing peak radioactivity were pooled, sterile filtered, and tested for binding and immunoreactivity (4). The purity was ≥90% as determined by thin-layer chromatography (TLC). The murine mAb had a specific activity up to 740 MBq/6.6 nmol (20 mCi/6.6 nmol) and an immunoreactivity of 50–80% (4).

The huA33 was also radioiodinated (^124^I/^131^I) as above (17) and had a purity of >98% as determined by TLC, a specific activity of 7.4 MBq/6.6 nmol (2 mCi/6.6 nmol), and an immunoreactivity of 78% (18). In another study, huA33 was radioiodinated with ^131^I, and the labeled antibody had a radiochemical purity of 99.6 ± 0.63% with an immunoreactivity of 63.8 ± 18.0%. The specific activity of this labeled mAb was not provided by the investigators (11).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=131I+A33+monoclonal+antibody+in+vitro)]

The cytotoxicity and subcellular distribution of radioiodinated murine mAb A33 was studied in a line of human colon cancer cells (19). The investigators showed that ^125^I/^131^I-labeled A33 was cytotoxic to the cells because the labeled A33 accumulated into the cytoplasmic vesicles and was transported close to the nucleus. Only 10% of the cells survived when they were exposed to 10 µCi/ml (370 kBq/ml) [^125^I]A33, but the survival increased to 90% when the cells were pretreated with a 100-fold excess of cold A33 and then exposed to 100 µCi/ml (3,700 kBq/ml) of the labeled antibody (19). Similar experiments performed with [^131^I]A33 showed it was toxic to the cells at either concentration given above.

In another study, Hoglund et al. investigated the in vitro cellular processing of [^125^I]huA33 in a human cancer cell line (20). The investigators observed that degradation of the intracellular antibody was slow, and an early loss of the label from the cells was caused by dissociation of the [^125^I]huA33 bound to the cell surface.

The in vitro properties of ^124^I-labeled huA33 were investigated with a human colorectal cell line, and the apparent association constant (K_a_) of the antibody was determined to be 2.2 × 10^9^ M^-1^ (18).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=+A33+monoclonal+antibody+rodentia+studies)]

With the use of positron emission tomography (PET), the biodistribution of [^124^I]huA33 was studied in xenografted mice (n = 5 animals/time point) bearing tumors from the human cancer cell line (18). The investigators observed uptake of the label (a total of six time points up to 240 h after the injection) mainly in the blood and various organs at 4 h, but by 24 h after injection the uptake was distinctly observed in the tumors. By 10 days after administration of the label, the radioactivity was localized primarily in the tumor and thyroid. The investigators did not perform blocking studies with cold huA33 (18).

The biodistribution of [^131^I]huA33 was investigated in nude mice bearing tumors from the human cancer cell line (21). Peak uptake of the label by the tumors was observed between 48 and 96 h with a mean uptake of 34% of the injected dose per gram of tissue. In these studies, specificity of antibody label uptake was determined by several techniques, including blocking by pretreatment of mice with unlabeled huA33. Using immunohistochemical techniques, the investigators demonstrated that a homogeneous distribution of the antibody in the tumors could be achieved in this model (21).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33+antibody+non-primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A33+antibody+non-human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=monoclonal+antibody+A33+human)]

The biodistribution and imaging characteristics of ^131^I-labeled murine mAb A33 were studied by Welt et al. in colorectal carcinoma patients with liver metastases (5). Imaging showed that the labeled antibody had a tumor tissue localization in 19 of 20 patients that correlated with surgical, pathological, and tissue radioactivity examination (5). One week after administration of the labeled antibody, the tumor/liver ratio ranged from 6.9/1 to 100/1 and the tumor/serum ratio ranged from 4.1/1 to 25.2/1. The isotope was visualized in the large bowel of some patients, but it was unclear if this represented specific antibody uptake or if it was gastric iodine secretion (5).

Only preliminary observations were obtained from a phase I/II study designed to determine the maximum tolerated dose (MTD) of murine [^131^I]A33 mAb (8). In this study, the localization of the labeled antibody in the metastized lesions of the patients was shown by single-photon emission computed tomography (SPECT) to last for at least 3 weeks after administration. The ^131^I-labeled antibody showed some hematological toxicity, but there was no toxicity in the bowel in spite of this being the only antigen-positive tissue in the body (8).

In another phase I/II study, also designed to determine the MTD of murine [^125^I]A33 mAb, SPECT analysis was performed on patients treated with the labeled antibody (4). Imaging revealed that the labeled antibody was located at all tumor sites identified by radiography. In this study, the MTD of the [^125^I]A33 mAb could not be established, and it was shown that the label was retained by the tumor tissue for up to 6 weeks after administration of the labeled antibody (4).

The biodistribution of [^131^I]huA33 was investigated in a phase I trial of patients with colorectal carcinomas (3). Imaging studies revealed that the label was distributed in the blood pool only during day 0 after administration, and there was distinct uptake in the colorectal carcinoma sites by up to the second day after the infusion. A similar uptake was also observed in the metastatic site of the liver and the lungs (3). A gradual clearance of the label through the bowel was observed in these patients.

A phase I dose escalation study of [^131^I]huA33 was performed in patients with pretreated metastatic colorectal carcinomas (10). Initially the label was distributed in the blood pool and then it was followed by tumor uptake and clearance through the bowel. In this study, whole-body planar images were acquired for all patients after infusion of the labeled antibody into the tumors, and persistent uptake of the antibody was observed up to 4 weeks after the infusion.

Sakamoto et al. investigated the in vivo characteristics of [^131^I]huA33 in patients with gastric carcinomas (11). Gamma imaging and ex vivo scintigraphy of the resected specimens showed a selective localization of the labeled antibody to the gastric cancer. From these observations the investigators concluded that the targeting characteristics of huA33 indicated it had a potential for the targeted treatment of advanced gastric carcinomas.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Heath J.K., White S.J., Johnstone C.N., Catimel B., Simpson R.J., Moritz R.L., Tu G.F., Ji H., Whitehead R.H., Groenen L.C., Scott A.M., Ritter G., Cohen L., Welt S., Old L.J., Nice E.C., Burgess A.W. (1997). The human A33 antigen is a transmembrane glycoprotein and a novel member of the immunoglobulin superfamily. Proc Natl Acad Sci U S A.
2 Ritter G., Cohen L.S., Nice E.C., Catimel B., Burgess A.W., Moritz R.L., Ji H., Heath J.K., White S.J., Welt S., Old L.J., Simpson R.J. (1997). Characterization of posttranslational modifications of human A33 antigen, a novel palmitoylated surface glycoprotein of human gastrointestinal epithelium. Biochem Biophys Res Commun.
3 Scott A.M., Lee F.T., Jones R., Hopkins W., MacGregor D., Cebon J.S., Hannah A., Chong G. (2005). P. U, A. Papenfuss, A. Rigopoulos, S. Sturrock, R. Murphy, V. Wirth, C. Murone, F.E. Smyth, S. Knight, S. Welt, G. Ritter, E. Richards, E.C. Nice, A.W. Burgess, and L.J. Old, A phase I trial of humanized monoclonal antibody A33 in patients with colorectal carcinoma: biodistribution, pharmacokinetics, and quantitative tumor uptake. Clin Cancer Res.
4 Welt S., Scott A.M., Divgi C.R., Kemeny N.E., Finn R.D., Daghighian F., Germain J.S., Richards E.C., Larson S.M., Old L.J. (1996). Phase I/II study of iodine 125-labeled monoclonal antibody A33 in patients with advanced colon cancer. J Clin Oncol.
5 Welt S., Divgi C.R., Real F.X., Yeh S.D., Garin-Chesa P., Finstad C.L., Sakamoto J., Cohen A., Sigurdson E.R., Kemeny N., et al. (1990). Quantitative analysis of antibody localization in human metastatic colon cancer: a phase I study of monoclonal antibody A33. J Clin Oncol.
6 Scott A.M., Welt S. (1997). Antibody-based immunological therapies. Curr Opin Immunol.
7 Tschmelitsch J., Barendswaard E., Williams C., Yao T.J., Cohen A.M., Old L.J., Welt S. (1997). Enhanced antitumor activity of combination radioimmunotherapy (131I-labeled monoclonal antibody A33) with chemotherapy (fluorouracil). Cancer Res.
8 Welt S., Divgi C.R., Kemeny N., Finn R.D., Scott A.M., Graham M., Germain J.S., Richards E.C., Larson S.M., Oettgen H.F., et al. (1994). Phase I/II study of iodine 131-labeled monoclonal antibody A33 in patients with advanced colon cancer. J Clin Oncol.
9 King D.J., Antoniw P., Owens R.J., Adair J.R., Haines A.M., Farnsworth A.P., Finney H., Lawson A.D., Lyons A., Baker T.S., et al. (1995). Preparation and preclinical evaluation of humanised A33 immunoconjugates for radioimmunotherapy. Br J Cancer.
10 Chong G., Lee F.T., Hopkins W., Tebbutt N., Cebon J.S., Mountain A.J., Chappell B., Papenfuss A., Schleyer P. (2005). P. U, R. Murphy, V. Wirth, F.E. Smyth, N. Potasz, A. Poon, I.D. Davis, T. Saunder, J. O'Keefe G, A.W. Burgess, E.W. Hoffman, L.J. Old, and A.M. Scott, Phase I trial of 131I-huA33 in patients with advanced colorectal carcinoma. Clin Cancer Res.
11 Sakamoto J., Oriuchi N., Mochiki E., Asao T., Scott A.M., Hoffman E.W., Jungbluth A.A., Matsui T., Lee F.T., Papenfuss A., Kuwano H., Takahashi T., Endo K., Old L.J. (2006). A phase I radioimmunolocalization trial of humanized monoclonal antibody huA33 in patients with gastric carcinoma. Cancer Sci.
12 Welt S., Ritter G., Williams C., Cohen L.S., John M., Jungbluth A., Richards E.A., Old L.J., Kemeny N.E. (2003). Phase I study of anticolon cancer humanized antibody A33. Clin Cancer Res.
13 Almqvist Y., Steffen A.C., Tolmachev V., Divgi C.R., Sundin A. (2006). In vitro and in vivo characterization of 177Lu-huA33: a radioimmunoconjugate against colorectal cancer. Nucl Med Biol.
14 Almqvist Y., Steffen A.C., Lundqvist H., Jensen H., Tolmachev V., Sundin A. (2007). Biodistribution of (211)at-labeled humanized monoclonal antibody a33. Cancer Biother Radiopharm.
15 Garin-Chesa P., Sakamoto J., Welt S., Real F.X., Rettig W.J., Old L.J. (1996). Organ-specific expression of the colon cancer antigen A33, a cell surface target for antibody-based therapy. Int J Oncol.
16 Catimel B., Nerrie M., Lee F.T., Scott A.M., Ritter G., Welt S., Old L.J., Burgess A.W., Nice E.C. (1997). Kinetic analysis of the interaction between the monoclonal antibody A33 and its colonic epithelial antigen by the use of an optical biosensor. A comparison of immobilisation strategies. J Chromatogr A.
17 Hunter W.M., Greenwood F.C. (1962). Preparation of iodine-131 labelled human growth hormone of high specific activity. Nature.
18 Lee F.T., Hall C., Rigopoulos A., Zweit J., Pathmaraj K., O'Keefe G.J., Smyth F.E., Welt S., Old L.J., Scott A.M. (2001). Immuno-PET of human colon xenograft- bearing BALB/c nude mice using 124I-CDR-grafted humanized A33 monoclonal antibody. J Nucl Med.
19 Daghighian F., Barendswaard E., Welt S., Humm J., Scott A., Willingham M.C., McGuffie E., Old L.J., Larson S.M. (1996). Enhancement of radiation dose to the nucleus by vesicular internalization of iodine-125-labeled A33 monoclonal antibody. J Nucl Med.
20 Hoglund J., Orlova A., Sundin A., Lundqvist H., Tolmachev V. (2006). Cellular processing in the SW1222 cell line of mAb A33 directly and indirectly radiohalogenated. Oncol Rep.
21 Barendswaard E.C., Scott A.M., Divgi C.R., Williams C., Coplan K., Riedel E., Yao T.J., Gansow O.A., Finn R.D., Larson S.M., Old L.J., Welt S. (1998). Rapid and specific targeting of monoclonal antibody A33 to a colon cancer xenograft in nude mice. International Journal of Oncology.